# IRDye800CW-Cyclic albumin-binding domain (Ac-RLIEDICLPRWGCLWEDDK-NH_2_)

Chemical name: | IRDye800CW-Cyclic albumin-binding domain (Ac-RLIEDICLPRWGCLWEDDK-NH_2_)
Abbreviated name: | IRDye800-cABD
Synonym:
Agent category: | Polypeptide
Target: | Albumin
Target category: | Acceptor
Method of detection: | Optical, near-infrared (NIR) fluorescence imaging
Source of signal: | IRDye 800CW
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4503491), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001963.2) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1950) for more information about human serum albumin (HSA).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=cABD%20IRDye800)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the natural background fluorescence interference of biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have a wider dynamic range and minimal background fluorescence as a result of reduced scattering compared with visible fluorescence detection. NIR fluorophores also have high sensitivity, resulting from low background fluorescence, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is a noninvasive alternative to radionuclide imaging in small animals or with probes in close proximity to the target in humans (4, 5). Among the various optical imaging agents, only indocyanine green (ICG (http://dailymed.nlm.nih.gov/dailymed/drugInfo.cfm?id=15096)), with NIR fluorescence absorption at 780 nm and emission at 820 nm, is approved by the United States Food and Drug Administration for clinical applications in angiography, blood flow evaluation, and liver function assessment. It is also under evaluation in several clinical trials (http://clinicaltrials.gov/ct2/results?term=indocyanine+green) for other applications, such as optical imaging and mapping of both the lymphatic vessels and lymph nodes in cancer patients for surgical dissection of tumors and endoscopic imaging of the pancreas and colon.

The primary function of the lymphatic system is to drain ~10% of the interstitial fluid from small capillaries to lymphatic vessels through lymph nodes and finally to the venous system (6-10). Lymph nodes form a natural filter for the lymphatic drainage and prevent the possible migration of cancer cells from the lymphatic system into the body. Serum proteins and macromolecules can be taken up by the large openings in the lymphatic capillaries. However, an accumulation of protein molecules may impair lymphatic flow and cause lymphedema and tissue edema. For NIR fluorescence imaging, ICG has been used in lymphatic imaging because of its association with serum proteins. However, ICG is degraded in aqueous conditions with a half-life of ~20 h and is sensitive to light (half-life, 2.3 h). IRDye 800CW (IRDye800) is an indocyanine-type NIR fluorophore with peak absorption at 785 nm and peak excitation emission at 803 nm, and it is about four-fold brighter than ICG. Dennis et al. (11) identified the peptide Ac-RLIEDICLPRWGCLWEDD (SA21), which bound with high affinity to human and murine serum albumin. Davies-Venn et al. (12) prepared a cyclic version of SA21 called cyclic albumin-binding domain (Ac-RLIEDICLPRWGCLWEDDK-NH_2_, cABD) and conjugated this with IRDye800 to form IRDye800-cABD for NIR fluorescence lymphatic imaging in mice.

### Related Resource Links:

- Chapters in MICAD (HSA (http://www.ncbi.nlm.nih.gov/books?term=human%20serum%20albumin%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (HSA (http://www.ncbi.nlm.nih.gov/gene/213))
- Articles in Online Mendelian Inheritance in Man (OMIM) (HSA (http://www.ncbi.nlm.nih.gov/omim/103600))
- Clinical trials (ICG (http://www.clinicaltrials.gov/ct2/results?term=ICG))
- Drug information in FDA (ICG (http://google2.fda.gov/search?q=Indocyanine+Green&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=4&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=cABD%20IRDye800%20and%20conjugation)]

Commercially available IRDye800-N-hydroxysuccinimide ester (LI-COR, Lincoln, NE) was used to conjugate cABD to form IRDye800-cABD, which was purified with gel filtration chromatography to a purity of 92%–98% (12). The molar ratio of IRDye800 to cABD was estimated to be 1.0 with mass spectroscopy. It has a molecular weight of 3.4 kDa. IRDye800-cABD has an extinction of coefficient of 171,000 M^–1^cm^–1^ and a quantum yield of 0.054 (excitation/emission, 784 nm/830 nm). It is more than four-fold brighter than ICG. IRDye800-cABD remained stable at both room temperature and 4°C for 15 d in phosphate-buffered saline or water. The log P values of IRDye800-cABD, ICG, and IRDye800 were –0.53, –0.69, and –1.13, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=cABD%20IRDye800%20and%20in%20vitro)]

The equilibrium dissociation constant (K_d_) value of cABD to mouse serum albumin was determined to be 65 ± 10 nM using surface plasmon resonance (12). The K_d_ value of conjugated cABD was 32 ± 5 nM. SDS-PAGE analysis showed that IRDye800-cABD bound at a 1:1 ratio to mouse serum albumin and to human serum albumin but not to ovalbumin.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=cABD%20IRDye800%20and%20rodentia)]

Davies-Venn et al. (12) compared the lymphatic clearance of ICG (10 µmol, n = 5), IRDye800 (2 µmol, n = 4), and IRDye800-cABD (2 µmol, n = 3) in female mice after intradermal injection at the base of the tail. The NIR fluorescence intensity within the region near the inguinal lymph node was measured at 0.5, 2.5, 15, 30, and 50 min after injection. ICG fluorescence intensities reached a plateau around 15–30 min and decreased to a lower level at 50 min. On the other hand, IRDye800 showed a decline from 2.5 min and reached a bottom at 30–50 min. ICG exhibited a trend of higher fluorescence intensities than IRDy800 at 15–50 min. IRDye800-cABD showed significantly higher fluorescence intensities than IRDy800 at 30 min and 50 min (P < 0.05). IRDye800-cABD showed a trend similar to ICG. The lymphatic vessels from the site of injection up to the inguinal lymph node and beyond were clearly visualized with NIR fluorescence imaging at 50 min after injection of ICG and IRDye800-cABD.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=cABD%20IRDye800%20and%20pig)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=cABD%20IRDye800%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=cABD%20IRDye800%20and%20human)]

No publication is currently available.

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Frangioni J.V. (2003). In vivo near-infrared fluorescence imaging. Curr Opin Chem Biol.
5 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
6 Clement O., Luciani A. (2004). Imaging the lymphatic system: possibilities and clinical applications. Eur Radiol.
7 Hoh C.K., Wallace A.M., Vera D.R. (2003). Preclinical studies of [(99m)Tc]DTPA-mannosyl-dextran. Nucl Med Biol.
8 Salem C.E., Hoh C.K., Wallace A.M., Vera D.R. (2006). A preclinical study of prostate sentinel lymph node mapping with [99mTC]diethylenetetramine pentaacetic acid-mannosyl-dextran. J Urol.
9 Styblo T., Aarsvold J.N., Grant S.F., Cohen C., Larsen T., Waldrop S., Alazraki N.P. (2001). Sentinel lymph nodes: optimizing success. Semin Roentgenol.
10 Vera D.R., Wallace A.M., Hoh C.K., Mattrey R.F. (2001). A synthetic macromolecule for sentinel node detection: (99m)Tc-DTPA-mannosyl-dextran. J Nucl Med.
11 Dennis M.S., Zhang M., Meng Y.G., Kadkhodayan M., Kirchhofer D., Combs D., Damico L.A. (2002). Albumin binding as a general strategy for improving the pharmacokinetics of proteins. J Biol Chem.
12 Davies-Venn, C.A., B. Angermiller, N. Wilganowski, P. Ghosh, B.R. Harvey, G. Wu, S. Kwon, M.B. Aldrich, and E.M. Sevick-Muraca, Albumin-Binding Domain Conjugate for Near-Infrared Fluorescence Lymphatic Imaging. Mol Imaging Biol, 2011